# Anti-intercellular adhesion molecule 1 antibody–conjugated gadolinium diethylenetriaminepentaacetic acid

Chemical name: | Anti-intercellular adhesion molecule 1 antibody–conjugated gadolinium diethylenetriaminepentaacetic acid
Abbreviated name: | Gd-DTPA-anti-ICAM-1 antibody
Synonym:
Agent Category: | Antibody
Target: | Intercellular adhesion molecule-1 (ICAM-1)
Target Category: | Antibody-ligand binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium
Activation: | Not required
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=4557877) sequence of human intercellular adhesion molecule 1 (ICAM-1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+conjugated+anti+ICAM+1+antibody)]

Inflammation is a protective response of infected or injured tissue and serves as a mechanism for the elimination of harmful substances and damaged tissues. It is characterized by localized capillary dilation, leukocyte infiltration, redness, and pain. Endothelial cells play a major role in the inflammation process, which is mediated and regulated by the interaction of a variety of molecules such as cytokines (chemoattractants and growth factors), low molecular weight mediators (leukotrienes, prostaglandins, and phospholipids), and adhesion molecules (selectins, integrins, and the intercellular adhesion molecule 1 (ICAM-1)) (1-3). The ICAM-1 (CD54) is a cell surface glycoprotein that is expressed by a variety of cell types including endothelial cells, activated leukocytes, and infiltrated macrophages. ICAM-1 and associated adhesion molecules are also the targets for various pathogenic viruses, bacteria, and parasites such as Plasmodium falciparum (1). Expression of membrane-bound ICAM-1 in inflammatory tissue is upregulated by proinflammatory cytokines such as IFN-γ and tumor necrosis factor α (TNF-α) under various conditions (4, 5). Because of its involvement and expression during the inflammation process, ICAM-1 has been targeted to visualize inflammatory tissue by magnetic resonance imaging (MRI).

Contrast agents for use with MRI are usually chelates of para- or superparamagnetic cations that belong to the lanthanide group of metals. In this regard a variety of contrast agents have been developed by the chelation of gadolinium (Gd) to different molecules, including proteins (6-8). To obtain a good contrast with MRI, it is important to have a high local concentration of the contrast agents in the target tissue before imaging. Antibodies or their fragments, directed toward specific cell surface markers, can serve as excellent molecules for the generation of MRI contrast agents because they can be labeled with metal ions with high efficiency (8). The metal-labeled antibody can then be used to perform MRI with great target specificity.

This chapter describes the in vitro and in vivo evaluation of an anti-ICAM-1 monoclonal antibody (MAb) bioconjugated to diethylenetriaminepentaacetic acid (DTPA) for MRI using a mouse inflammation model (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+synthesis+)]

A rat hybridoma (unspecified by the investigators) was obtained from ATCC (http://atcc.org/common/catalog/numSearch/numResults.cfm) and used for production of the anti-ICAM-1 MAb. The MAb was purified from the culture supernatant by affinity chromatography. Identification of the MAb by sodium dodecyl sulphate polyacrylamide gel electrophoresis and Western blot analysis confirmed the presence of the heavy (50 kDa) and light (25 kDa) chains of the MAb in the purified preparation (9).

For bioconjugation of the MAb with DTPA, DTPA bisanhydride was dissolved in dimethylformamide and added to the MAb solution in phosphate-buffered saline (pH 8.5) (9). The reaction was performed for 1 h at room temperature and the DTPA-conjugated MAb was purified on a Sephadex G-25 (PD-10) column.

To generate a gadolinium (Gd) complex of the DTPA–anti-ICAM1 antibody, Gd chloride (GdCl_3_) was dissolved in water and added to a solution of the DTPA-MAb in sodium acetate buffer (pH 5.5) at a ratio of 40:1 (9). The solution was loaded on a PD-10 column to remove excess GdCl_3_ The Gd-DTPA MAb complex was analyzed using matrix-assisted laser desorption ionization–time of flight (MALDI-TOF), and the Gd content was determined with inductively coupled plasma mass spectrometry (ICP-MS) (9). Conjugation of the antibody with DTPA and Gd was evident from the increase in molecular weight observed during MALDI-TOF analysis. An ICP-MS analysis revealed that the conjugate had a molar ratio of 20 ± 3 Gd per IgG molecule. From the conjugation procedure the DTPA-antibody complex yield was 95% and the Gd-DTPA antibody complex yield was 80%.

For use as a control, an immunoglobulin (IgG) was conjugated to DTPA and Gd, as detailed above, to obtain Gd-DTPA-IgG. As another control, Gd-DTPA was also used in a study; however, the authors did not mention its source or if it was synthesized in the laboratory (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+in+vitro)]

Binding of Gd-DTPA-anti-ICAM1 antibody to ICAM-1 was investigated by using MS-1 cells (these have an endothelial origin) stimulated with TNF-α, a potent inducer of ICAM-1 on endothelial cells (9). As a control, HT1080 cells were exposed to the conjugated MAb with or without exposure to TNF-α. The binding was determined in the presence or absence of the anti-ICAM-1 MAb that served as a competitive inhibitor for the Gd-DTPA–conjugated MAb. To reduce non-specific phagocytosis of the contrast agent, the study was performed at 4°C and the anti-ICAM-1 MAb was added at twice the concentration of the Gd-DTPA-anti-ICAM-1 MAb.

Induction of ICAM-1 on the MS-1 cells by TNF-α was confirmed with immunoblot analysis. Using the same technique it was shown that HT1080 cells had no ICAM-1 induction upon exposure to TNF-α. The binding of Gd-DTPA-ICAM-1 MAb to the cells was determined with MRI of the cells and measurement of the T_1_ signal. A determination of the contrast/noise ratios (CNR) showed there was a nearly two-fold increase in the ratio only for the TNF-α–stimulated MS-1 cells after exposure to the cytokine. During the same period, the other cells (MS-1 cells + TNF-α, MS-1 cells + TNF-α + anti-ICAM-1 MAb, and HT1080 cells with or without TNF-α stimulation) showed little change in the CNR. The increase in T_1_ signal only for the MS-1 cells exposed to TNF-α indicated that the Gd-DTPA–conjugated MAb was potentially useful as an in vivo inflammation-targeted contrast agent (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+rodents)]

A mouse inflammation model was used to evaluate the use of Gd-ICAM-1 MAb for the imaging of inflammation (9). Acute inflammation was generated in the mouse thigh by injection of Staphylococcus aureus into the thigh muscle, and the T_1_ intensity of the inflammatory tissue was determined 24 h after injection using the Gd-ICAM-1 MAb. The T_1_ signal of the conjugated MAb was compared to that obtained with Gd-DTPA and Gd-DTPA-IgG. With Gd-DTPA, an increase in the T_1_ relaxivity was noticed at the site of inflammation within 1 min of injection and it disappeared after 1 h. The Gd-DTPA-IgG did not show an enhancement of T_1_ up to 24 h after the injection, the last observation time point reported. With the Gd-DTPA-anti-ICAM-1 MAb, an increase in the T_1_ signal was evident within 30 min and it increased in the inflammatory tissue up to 24 h after injection (~three-fold higher than Gd-DTPA alone). This indicated that the metal-labeled MAb accumulated at the site of inflammation during this period. It was also observed that, although 10-fold less Gd-DTPA-ICAM-1 MAb (9 nmol Gd/g body weight) compared to Gd-DTPA (100 nmol Gd/g body weight) was administered to the mice, Gd-DTPA-ICAM-1 displayed ~three-fold higher T_1_ signal enhancement compared to Gd-DTPA. Changes in the T_1_ signal of mice injected with the Gd-DTPA-ICAM-1 MAb was also monitored up to 11 days after injection. A sigmoidal decay of the T_1_ signal was observed at the inflammation site in these animals during this period.

The investigators concluded that the Gd-DTPA-ICAM-1 MAb was suitable to study inflammation with MRI in a mouse abscess model (9). However, the authors cautioned that immunoglobulins can cause an immune reaction in animals and humans. To reduce this possibility, the authors suggested it would be best to modify the immunoglobulin by using an F(ab’) antibody fragment for such investigations.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-DTPA+anti-ICAM-1+antibody+human+studies)]

No publications are currently available.

## References

1 Hopkins A.M., Baird A.W., Nusrat A. (2004). ICAM-1: targeted docking for exogenous as well as endogenous ligands. Adv Drug Deliv Rev.
2 Hansson G.K. (2005). Inflammation, atherosclerosis, and coronary artery disease. N Engl J Med.
3 Winsauer G., de Martin R. (2007). Resolution of inflammation: intracellular feedback loops in the endothelium. Thromb Haemost.
4 Bevilacqua M.P. (1993). Endothelial-leukocyte adhesion molecules. Annu Rev Immunol.
5 Vachula M., Van Epps D.E. (1992). In vitro models of lymphocyte transendothelial migration. Invasion Metastasis.
6 Artemov D., Mori N., Ravi R., Bhujwalla Z.M. (2003). Magnetic resonance molecular imaging of the HER-2/neu receptor. Cancer Res.
7 Poduslo J.F., Curran G.L., Peterson J.A., McCormick D.J., Fauq A.H., Khan M.A., Wengenack T.M. (2004). Design and chemical synthesis of a magnetic resonance contrast agent with enhanced in vitro binding, high blood-brain barrier permeability, and in vivo targeting to Alzheimer's disease amyloid plaques. Biochemistry.
8 Artemov D., Bhujwalla Z.M., Bulte J.W. (2004). Magnetic resonance imaging of cell surface receptors using targeted contrast agents. Curr Pharm Biotechnol.
9 Choi K.S., Kim S.H., Cai Q.Y., Kim S.Y., Kim H.O., Lee H.J., Kim E.A., Yoon S.E., Yun K.J., Yoon K.H. (2007). Inflammation-specific t(1) imaging using anti-intercellular adhesion molecule 1 antibody-conjugated gadolinium diethylenetriaminepentaacetic Acid. Mol Imaging.